# Gd@C_82_ Fullerenol

Chemical name: | Gd@C_82_ Fullerenol
Abbreviated name: | Gd@C_82_(OH)_40_
Synonym: | Gd-fullerenol
Agent category: | Cage molecule
Target:
Target category: | Retention
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd@C82 + fullerenol)]

Fullerenes, also known as buckyballs, are spheroidal carbon cages with a molecular formula of C_2n_ (n = 30–41) and a diameter of ~1 nm (1). The high chemical stability of fullerenes can resist any potential metabolic cage-opening process and hence prevents them from degradation in various biological conditions (2). Fullerenes contain hollow interiors that can hold atoms or ions as payloads for various biomedical applications (1). For example, Gd atoms or the trimetallic nitride Gd_3_N can be trapped inside the cage to form endohedral metallofullerenes denoted as Gd@C_2n_ or Gd_3_N@C_2n_, where the “@” symbol refers to the encapsulated nature of the Gd or Gd_3_N. For the Gd@C_2n_, the encapsulation of electropositive Gd atom leads to the transfer of electrons from the Gd atom to the electronegative fullerene cage, resulting in a zwitterion [Gd^3+^@C_82_^3-^]. For Gd_3_N@C_2n_, each Gd atom shares one electron with the N atom and donates the other two electrons to the C80 cage that is in I_h_-symmetry to produce a zwitterion [Gd_3_N^6+^@C_80_^6-^] (3, 4). These endohedral metallofullerenes thus lead to the generation of a novel type of contrast agent for magnetic resonance imaging (MRI), which possesses a high biological safety in that the carbon cage completely prevents the release of toxic Gd^3+^ ions into surrounding tissues (5, 6). The surface of fullerenes can be functionalized with a variety of groups or specific ligands; i.e., the addition of hydroxyls or polyethylene glycols (PEG) substantially increases their aqueous solubility (7).

Gd-Fullerenols (Gd@C_82_(OH)_40_) are water-soluble Gd endohedral metallofullerenes used with in vivo MRI (8). The encapsulation of Gd has three electrons transferred to the C82 fullerene cage, resulting in zwitterions [Gd^3+^@C_82_(OH)_40_^3-^] in which seven unpaired electrons are located on the 4f-orbital of gadolinium ion and one unpaired electron is located on the fullerene cage. These unpaired electrons contribute to the paramagnetic moment of Gd@C_82_(OH)_40_. Nevertheless, the encapsulation of the Gd ion inside the carbon cage prevents direct coordination and exchange of water to Gd^3+^. The relaxation enhancement of Gd@C_82_(OH)_40_ is therefore quite different from the classic inner-sphere mechanism in conventional Gd chelates such as Gd-DTPA but depends on its paramagnetic moment and intermolecular aggregation effect (1). The aggregation leads to an increase in the rotational correlation time and alterations in the water exchange kinetics, which both influence the resultant relaxivity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd@C82 + fullerenol)+AND+synthesis%0D%0A)]

Mikawa et al. reported the preparation of Gd@C_82_(OH)_n_ in two steps (8). Initially, Gd@C_82_ was obtained by arc-vaporization of 0.8% Gd/graphite rods under helium atmosphere (50 Torr), followed by extraction with carbon disulfide and then purification with high-performance liquid chromatography. The purified Gd@C_82_ was dissolved in toluene and reacted with 50% aqueous NaOH solution in the presence of 15-crown-5 as a catalyst at room temperature to produce brownish Gd@C_82_(OH)_n_. The average number of hydroxyl groups (n) was found to be ~40, yielding a molecular formula of Gd@C_82_(OH)_40_ (one Gd atom per fulluerene). The charge state of encapsulated gadolinium atom was found to be trivalent (Gd^3+^) using a Gd M_4,5_-edge electron energy loss spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd@C82 + fullerenol)+AND+%22in+vitro%22)]

The proton relaxivity of Gd@C_82_(OH)_40_ was measured in aqueous solutions with various magnetic fields. The T_1_ relaxivity (R_1_) was 67 mM^-1^s^-1^ at 0.47 T, 81 mM^-1^s^-1^ at 1.0 T, and 31 mM^-1^s^-1^ at 4.7 T. The T_2_ relaxivity (R_2_) was 79 mM^-1^s^-1^ at 0.47 T, 108 mM^-1^s^-1^ at 1.0 T, and 131 mM^-1^s^-1^ at 4.7 T. Compared to the 3.9 mM^-1^s^-1^ (R_1_) and 6.2 mM^-1^s^-1^ (R_2_) of Gd-DTPA at 1.0 T, the relaxivity of Gd@C_82_(OH)_40_ (R_1_ or R_2_) was increased ~20-fold. In addition, the relaxivity of Gd@C_82_(OH)_40_ appeared to be significantly influenced by the pH and ionic strength in the solution; i.e., a bell shape profile was observed for T_1_ relaxivity in the pH range of 3–8, and T_1_ relaxivity was lower in a 1.0 M aqueous NaCl solution than in water (61 mM^-1^s^-1^versus 67 mM^-1^s^-1^).

Anderson et al. used Gd@C_82_(OH)_40_ to label human cervical carcinoma cells (HeLa) and human mesenchymal stem cells (MSCs) (9). Cells were incubated for 10 h with 0.5 μmol Gd/ml Gd@C_82_(OH)_40_ in the presence of the transfection agent protamine sulfate. The labeled cells exhibited ~100% labeling efficiency and viability with cellular Gd content of 1.19 × 10^-10^ mg per cell (7.5 × 10^-13^ mmol Gd per cell). The cellular proliferation was evaluated with 3-(4,5-[underlined: di] (http://en.wikipedia.org/wiki/Di-) [underlined: methyl] (http://en.wikipedia.org/wiki/Methyl) [underlined: thiazol] (http://en.wikipedia.org/wiki/Thiazole)-2-yl)-2,5-di[underlined: phenyl] (http://en.wikipedia.org/wiki/Phenyl)tetrazolium bromide (MTT) assay; the MTT ratio was 74–78% for day 2 through day 6 and ~100% by day 9. The internalized Gd@C_82_(OH)_40_ nanoparticles were found with electron microscopy to be aggregated within the endosomes in cytoplasm. In addition, the labeled MSCs demonstrated normal adipogenic, chondrogenic, and osteogenic differentiation compared with the unlabeled control cells. The relaxation enhancement efficiency was examined ex vivo in the labeled HeLa cells with a 7-T MR imager. An increase of ~200% in the signal intensity was observed in the T_1_-weighted images compared to unlabeled cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd@C82 + fullerenol) +AND++rodentia)]

Mikawa et al. examined the biodistribution of Gd@C_82_(OH)_40_ in mice with in vivo MRI, followed by Gd assay with inductively coupled plasma-atomic emission spectrometry (ICP-AES) (8). CDF1 mice (n = 3, 8 wks old, ~20 g) were injected intravenously with Gd@C_82_(OH)_40_ at a dose of 5 μmol Gd/kg (compared to the typical dose of 100 μmol Gd/kg for Gd-DTPA). T_1_-Weighted images were collected with a 4.7-T imager before injection and at 30 min, 1 h, and 24 h after injection. Strong signal enhancement was observed in the lung, liver, spleen, and kidney. The Gd content in these organs was quantified with ICP-AES: ~60 μg Gd/g tissue in the lung, ~8 μg Gd/g tissue in the liver, ~5 μg Gd/g tissue in the spleen, and ~3 μg Gd/g tissue in the blood at 30 min; ~25 μg Gd/g tissue in the lung, ~10 μg Gd/g tissue in the liver, ~8 μg Gd/g tissue in the spleen, and <2 μg Gd/g tissue in the blood at 1 h; <1 μg Gd/g tissue in the lung, ~9 μg Gd/g tissue in the liver, ~12 μg Gd/g tissue in the spleen, and fell into background in the blood at 24 h. These results demonstrated that Gd@C_82_(OH)_40_ was readily trapped in the reticuloendothelial system.

Anderson et al. examined the relaxation enhancement efficiency of Gd@C_82_(OH)_40_-labeled cells in vivo with MRI (9). Rats were injected intramuscularly with 3 × 10^6^ Gd@C_82_(OH)_40_-labeled MSCs in the thigh and imaged with a 7-T imager. A 33% increase in imaging contrast versus muscle was observed in the T_1_-weighted images. As a comparison, a rat was injected intramuscularly with 4 × 10^6^ Gd@C_82_(OH)_40_-labeled MSCs (~1.19×10^-10^ mg Gd per cell or 7.5× 10^-13^ mmol Gd per cell) in the thigh and imaged at 1.5 T. These labeled cells demonstrated an 83% increase in signal intensity compared to the muscle in the T_1_-weighted images.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( Gd@C82 + fullerenol) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd@C82 + fullerenol) +AND+human)]

No publication is currently available.

### NIH Support

NIH intramural Research Program.

## References

1 Bolskar R.D. (2008). Gadofullerene MRI contrast agents. Nanomed.
2 Fatouros P.P., Corwin F.D., Chen Z.J., Broaddus W.C., Tatum J.L., Kettenmann B., Ge Z., Gibson H.W., Russ J.L., Leonard A.P., Duchamp J.C., Dorn H.C. (2006). In vitro and in vivo imaging studies of a new endohedral metallofullerene nanoparticle. Radiology.
3 Aihara J. (2001). Kinetic stability of metabllofullerenes as predicted by bond resonance enery model. Phys. Chem. Chem. Phys.
4 Ge Z., Duchamp J.C., Cai T., Gibson H.W., Dorn H.C. (2005). Purification of endohedral trimetallic nitride fullerenes in a single, facile step. J Am Chem Soc.
5 Lu J., Sabirianov R.F., Mei W.N., Gao Y., Duan C.G., Zeng X. (2006). Structural and magnetic properties of Gd3N@C80. J Phys Chem B.
6 Krause M., Dunsch L. (2005). Gadolinium nitride Gd3N in carbon cages: the influence of cluster size and bond strength. Angew Chem Int Ed Engl.
7 MacFarland D.K., Walker K.L., Lenk R.P., Wilson S.R., Kumar K., Kepley C.L., Garbow J.R. (2008). Hydrochalarones: a novel endohedral metallofullerene platform for enhancing magnetic resonance imaging contrast. J Med Chem.
8 Mikawa M., Kato H., Okumura M., Narazaki M., Kanazawa Y., Miwa N., Shinohara H. (2001). Paramagnetic water-soluble metallofullerenes having the highest relaxivity for MRI contrast agents. Bioconjug Chem.
9 Anderson S.A., Lee K.K., Frank J.A. (2006). Gadolinium-fullerenol as a paramagnetic contrast agent for cellular imaging. Invest Radiol.